# Methyl 2-(2-[^18^F]fluoro-4-nitrobenzamido)-3-methylbutanoate

Chemical name: | Methyl 2-(2-[^18^F]fluoro-4-nitrobenzamido)-3-methylbutanoate
Abbreviated name: | [^18^F]MFNBMB
Synonym: | [^18^F]1
Agent Category: | Compound
Target: | Tumors
Target Category: | Nonspecific tissues
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | [^18^F]
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure of [^18^F]MFNBMB for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=MFNBMB)]

The most commonly used radiochemical for positron emission tomography (PET) imaging of brain or systemic cancerous tumors is 2-[^18^F]fluorodeoxyglucose ([^18^F]FDG), a United States Food and Drug Administration approved imaging agent, but the use of this radiolabel is not without limitations because, among several application drawbacks, it tends to produce a high background in the brain and inflamed tissues during imaging (1, 2). To circumvent problems encountered with [^18^F]FDG, some investigators developed and evaluated unnatural amino acid (aa) derivatives such as O-2-[^18^F]fluoroethyl-L-tyrosine (L-[^18^F]FET) for the detection of tumors, particularly of the brain, and it was shown that L-[^18^F]FET was superior to [^18^F]FDG in distinguishing tumors from inflammation (3). However, the synthesis of ^18^F-labeled aa is cumbersome and, because an electrophilic substitution reaction is used to introduce the label into the aa, the final labeled product yields are very low (2). An alternative synthetic method of placing a fluoroalkyl group on the aromatic ring of tyrosine was observed to improve the yield of L-[^18^F]FET, but it prolonged the synthesis time for the radiochemical (4, 5). In an effort to simplify the synthesis of ^18^F-radiolabeled aas, ^18^F-labeled fluoroarylvaline derivatives of L-valine were prepared after modifying the aa with 2,4-dinitrobenzoic acid (2). According to the investigators, introduction of ^18^F at the ortho-position of 2,4-dinitrobenzoic acid is very easy, and the attachment of this moiety to L-valine results in an improved lipophilicity of the molecule. Using this method, two derivatives of L-valine were produced: methyl 2-(2-[^18^F]fluoro-4-nitrobenzamido)-3-methylbutanoate ([^18^F]MFNBMB; [^18^F]1) and methyl 2-(2-[^18^F]fluoro-4-nitrobenzamido)-3-methylbutanoic acid ([^18^F]FNBMBA; [^18^F]2) (2). These radiotracers were evaluated under in vivo conditions, and their biological properties were compared with those of [^18^F]FDG and L-[^18^F]FET. This chapter describes the characteristics of [^18^F]MFNBMB and its biodistribution in tumor-bearing mice. The characteristics of [^18^F]FNBMBA and its biodistribution in tumor-bearing mice is described in a separate chapter of MICAD (6).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=MFNBMB+synthesis)]

The synthesis of MFNBMB, with a yield of 66%, was detailed by Qiao et al. (2). Radiolabeling of MFNBMB to obtain [^18^F]MFNBMB was performed using a nucleophilic substitution denitrofluorination reaction as described elsewhere (2). The radiochemical yield of the synthesis was ~30–40% without decay correction, with chemical and radiochemical purity of >99%, respectively. The time required for the synthesis was ~100 min. The specific activity of the labeled compound was not reported.

[^18^F]MFNBMB was reported to be 100% stable, as determined with thin-layer chromatography and high-performance liquid chromatography (HPLC) in normal saline, phosphate-buffered saline (pH not reported), or 96% ethanol for up to 6 h at room temperature, and in ethanol, dimethylformamide, and acetonitrile for up to 30 min at 60°C (2). HPLC analysis of blood obtained from mice 30 min after treatment with [^18^F]MFNBMB showed that the radiolabeled compound was also stable under in vivo conditions.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=MFNBMB+in+vitro)]

No references are currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=MFNBMB+rodentia)]

The biodistribution of [^18^F]MFNBMB was investigated in mice bearing mouse sarcoma S180 cell tumors (2). The mice were injected with the radiolabeled compound through the tail vein, and the animals were euthanized at 5, 15, 30, 60, and 120 min (n = 4 animals/time point) after treatment. The tumor and other organs of interest were removed from the animals, and accumulated radioactivity was measured with a gamma counter (represented as percent of injected dose/gram tissue (% ID/g)). A rapid distribution of radioactivity in the various organs and tissue, within 5 min of injection, was observed. In general, by 120 min after the treatment a decrease in accumulated radioactivity was reported in all organs and tissue, including tumors. The tumor/blood ratio increased from 0.90 at 5 min to 3.44 at 60 min, and then decreased to 1.67 at 120 min. The tumor/brain ratio increased from 2.79 at 5 min to 7.06 at 30 min, and then decreased to 2.61 at 120 min. A similar trend was also noted for the tumor/muscle ratio of the animals. The tumor/blood, tumor/brain, and tumor/muscle ratios with [^18^F]MFNBMB were lower than those obtained with [^18^F]FNBMBA (for comparison, see the MICAD chapter regarding [^18^F]FNBMBA (6)).

For comparison, a similar biodistribution study was also performed with the tumor-bearing mice using [^18^F]FDG and L-[^18^F]FET, respectively (2). The blood clearance of both [^18^F]MFNBMB and [^18^F]FNBMBA were reported to be slower than that of [^18^F]FDG, but faster than that of L-[^18^F]FET. Compared with [^18^F]MFNBMB, [^18^F]FNBMBA, or L-[^18^F]FET, the tumor/blood ratio for [^18^F]FDG increased from 1.17 at 5 min to 15.85 at 120 min. However, the tumor/brain ratio of [^18^F]FDG was much lower at all time points (0.53–1.33) than that of the other three labeled compounds (2.79–2.61 for [^18^F]MFNBMB, 9.38–6.90 for [^18^F]FNBMBA, and 2.10–2.95 for L-[^18^F]FET). The tumor/muscle ratios of [^18^F]FDG and L-[^18^F]FET (0.81 and 0.72, respectively, at 5 min after injection) increased up to 120 min (2.20 for [^18^F]FDG and 1.40 for L-[^18^F]FET). In comparison, the ratios for [^18^F]MFNBMB and [^18^F]FNBMBA decreased from 1.94 and 1.38, respectively, at 5 min to 0.54 and 0.66, respectively, at 120 min.

From these studies, the investigators concluded that [^18^F]MFNBMB was superior to both [^18^F]FDG and L-[^18^F]FET for the detection of brain tumors in mice. However, no studies were reported to investigate if the metabolic pathway followed by [^18^F]FNBMBA was the same as valine, its parent compound.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=MFNBMB+Non-Primate+Mammals)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=MFNBMB+Non-Human+Primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=MFNBMB+Human+Studies)]

No references are currently available.

## Supplemental Information

[Disclaimer]

No information is currently available.

## References

1 Dunphy M.P., Lewis J.S. (2009). Radiopharmaceuticals in preclinical and clinical development for monitoring of therapy with PET. J Nucl Med.
2 Qiao Y., He Y., Zhang S., Li G., Liu H., Xu J., Wang X., Qi C., Peng C. (2009). Synthesis and evaluation of novel F-18 labeled fluoroarylvaline derivatives: potential PET imaging agents for tumor detection. Bioorg Med Chem Lett.
3 Lee T.S., Ahn S.H., Moon B.S., Chun K.S., Kang J.H., Cheon G.J., Choi C.W., Lim S.M. (2009). Comparison of 18F-FDG, 18F-FET and 18F-FLT for differentiation between tumor and inflammation in rats. Nucl Med Biol.
4 Heiss P., Mayer S., Herz M., Wester H.J., Schwaiger M., Senekowitsch-Schmidtke R. (1999). Investigation of transport mechanism and uptake kinetics of O-(2-[18F]fluoroethyl)-L-tyrosine in vitro and in vivo. J Nucl Med.
5 Wester H.J., Herz M., Weber W., Heiss P., Senekowitsch-Schmidtke R., Schwaiger M., Stocklin G. (1999). Synthesis and radiopharmacology of O-(2-[18F]fluoroethyl)-L-tyrosine for tumor imaging. J Nucl Med.
6 Chopra, A., Methyl 2-(2-[18F]fluoro-4-nitrobenzamido)-3-methylbutanoate. [[18F]FNBMBA]. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.